# Id protein-firefly luciferase N-fragment & firefly luciferase C-fragment-MyoD protein

Chemical name: | Id protein- firefly luciferase N-fragment & firefly luciferase C-fragment-MyoD protein
Abbreviated name: | Id-NFluc & CFluc-MyoD
Synonym:
Agent category: | Protein
Target: | Other
Target category: | Other –protein-protein interaction
Method of detection: | Optical Imaging
Source of signal/contrast: | Luciferin
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MyoD + Fluc +ID)]

Firefly luciferase (Fluc) is an oxygenase extracted from Photinus pyralis with a molecular weight of 62 kDa (1). In the presence of adenosine triphosphate (ATP) and O_2_, Fluc oxidizes the heterocyclic substrate D-luciferin to oxyluciferin and emits light in the wavelength range of 400–620 nm (2). The active site of Fluc comprises two distinct domains, a large N-terminal domain (residue 4–436) and a small C-terminal domain (residue 440–544), which are separated by a wide cleft (1). Splitting Fluc into N- and C-terminal fragments destroys its enzymatic activity, resulting in a complete loss of bioluminescence. The enzymatic activity or bioluminescence can be restored if the N- and C-terminal fragments are in close proximity (3). This led to the development of a novel labeling strategy for imaging protein–protein interactions in vivo, the split reporter (4). In this method, reporters like Fluc are dissected into two fragments and fused to a pair of proteins (A and B) that strongly interact with each other. The enzymatic activity of Fluc can be restored via two split reporter approaches: a complementation strategy and a reconstitution strategy. In the complementation strategy, protein A is connected with the N-terminal fragment of Fluc, and protein B is connected with the C-terminal fragment of Fluc. Interaction between protein A and B recovers the enzymatic activity of Fluc by bringing the two fragments of Fluc closely together. In the reconstitution strategy, protein A is connected with the N-terminal of one-half of a protein splicing system such as DNA polymerase III (N-intein DnaE) followed by N-terminal fragment of Fluc. Protein B is linked to the C-terminal of the other half of the splicing system (C-intein DnaE) followed by the C-terminal fragment of Fluc. The interaction between protein A and B brings the N- and C-inteins together, resulting in the joining of N- and C-terminal fragments of Fluc by a peptide bond and a release of a fully reconstituted protein Fluc. Both split enzyme approaches allow for recovery of bioluminescence.

MyoD is a myogenic regulatory protein that belongs to the basic helix-loop-helix (bHLH) family of transcription factors (5). MyoD activates myogenesis by binding directly to the control region of muscle-specific genes, and it converts fibroblasts into skeletal muscle. The helices in MyoD bind tightly with other HLH factors such as Id to form a heterodimer. Id, also known as an inhibitor of differentiation or inhibitor of DNA binding, lacks the basic domain for DNA binding and acts as dominant negative regulator in myogenesis or other cell proliferations (6). Id protein-firefly luciferase N-fragment & firefly luciferase C-fragment-MyoD protein (Id-NFluc & CFluc-MyoD) make up a pair of interacting proteins attached to the split Fluc fragments (7). Id-NFluc & CFluc-MyoD can be prepared with complementation strategy or reconstitution strategy, and are employed for in vivo imaging of the interaction between Id and MyoD via the produced bioluminescence.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(MyoD + Fluc + ID)+AND+synthesis%0D%0A)]

Paulmurugan et al. briefly described the preparation of Id-NFluc & CFluc-MyoD via the complementation strategy or reconstitution strategy (7). In the complementation strategy, four plasmid vectors were constructed. First, the N-part of the Fluc gene with the linker peptide FFAGYC at its C-terminus was released from the vector pIRES DSL(Y/S) by NheI and HindIII restriction enzymes, followed by ligation to the pcDNA 3.1(+) vector backbone to product the plasmid vector pCMV-NFluc via an RNA polymerase II-type human cytomegalovirus (CMV) promoter. Second, the cDNA of the Id gene was released by BamHI and Xhol from a vector containing pBIND-Id and cloned in the C-terminal of pCMV-NFluc to generate the vector pCMV-NFluc-Id. Third, the polymerase chain reaction (PCR)-amplified fragment of Cfluc containing the start codon was cloned in the NheI and XhoI site of pcDNA 3.1 to generate the vector pCMV-CFluc. Finally, the PCR-amplified fragment of MyoD with the start codon was ligated to pcDNA 3.1(+) in NheI/BamHI site and further inserted with the PCR product of Cfluc with the linker peptide CLKS in the BamHI and XhoI site to construct the vector pCMV-MyoD-CFluc. The obtained vectors pCMV-NFluc-Id, pCMV-MyoD-CFluc, and pCMV-NFluc-Id plus pCMV-MyoD-CFluc were used to transfect cells to examine the efficiency of the complementation strategy. In the complementation strategy, two plasmid vectors were constructed. First, the N-half of DnaE was PCR-amplified by using the template pIRES DSL(Y/S) and cloned in the HindIII site of vector PC to construct the vector pCMV-NFluc-DnaE-n-Id. Then, the PCR-amplified C-half of DnaE was cloned at the BamHI site of the vector pCMV-MyoD-CFluc to construct the vector pCMV-MyoD-DnaE-c-CFluc. The obtained vectors pCMV-NFluc-DnaE-n-Id, pCMV-MyoD-DnaE-c-Cfluc, and pCMV-NFluc-DnaE-n-Id plus pCMV-MyoD-DnaE-c-CFluc were used to transfect cells to examine the efficiency of the reconstitution strategy. As a control, the Fluc gene released from the vector pNFkB-Fluc by NheI and XhoI to pcDNA 3.1(+) was used to produce pCMV-Fluc.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( MyoD + Fluc + ID)+AND+%22in+vitro%22)]

The efficiency of the complementation strategy was evaluated in vitro (7). COS-1, N_2a_, and 293T cells were transfected with individual vectors alone (pCMV-NFluc-Id or pCMV-MyoD-CFluc), or cotransfected with both vectors (pCMV-NFluc-Id plus pCMV-MyoD-CFluc). The proteins secreted from these cells were exposed to the D-luciferin substrate followed by bioluminescence measurements. After a transient transfection with the individual vectors, the enzymatic activity was significantly lower compared with the full reporter Fluc; ~25-fold reduction was found in NFluc and >1,000-fold reduction in CFluc. After a transient cotransfection with both vectors, a higher enzymatic reactivity was observed, which increased 15 ± 5-fold compared to the NFluc or 500 ± 50-fold compared to the CFluc. This result demonstrated a ~40–60% efficiency with the complementation strategy compared to the full reporter Fluc. As a control, the Id portion in the vector pCMV-NFluc-Id was substituted with p53. The produced vector pCMV-NFluc-p53 led to a secretion of NFluc-p53, a protein that did not interact with MyoD. After a transient cotransfection of pCMV-NFluc-p53 plus pCMV-MyoD-CFluc, the enzymatic activity was found to be 100 times less than that from a pair of interaction proteins produced by cotransfection of pCMV-NFluc-Id plus pCMV-MyoD-CFluc.

The efficiency of the reconstitution strategy was also evaluated in vitro (7). COS-1, N_2a_, and 293T cells were transfected with individual vectors alone (pCMV-NFluc-DnaE-n-Id or pCMV-MyoD-DnaE-c-CFluc), or cotransfected with both vectors (pCMV-NFluc-DnaE-n-Id plus pCMV-MyoD-DnaE-c-CFluc). After a transient transfection, the secreted proteins were exposed to the D-luciferin substrate followed by bioluminescence measurements. The insertion of intein DnaE appeared to have no effect on the enzymatic activity in all cell lines. After a transient cotransfection with both vectors, the enzymatic activity was found to be 45–50% compared to the full reporter Fluc. Western blot analysis demonstrated that a full Fluc protein was recovered. As a control, cells were also cotransfected with pCMV-NFluc-DnaE-n-p53 plus pCMV-MyoD-DnaE-c-CFluc, which secreted a pair of non-interacting proteins (p53 and MyoD). No apparent enzymatic activity was found with this pair of proteins.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( MyoD + Fluc + ID) +AND++rodentia)]

The effect of the complementation strategy was examined in mice in vivo (7). 293T cells were transiently transfected with individual vectors alone (pCMV-NFluc-Id or pCMV-MyoD-CFluc), or cotransfected with both vectors (pCMV-NFluc-Id plus pCMV-MyoD-CFluc). An aliquot of 1 × 10^6^ cultured transfected cells were implanted subcutaneously in different sites in anesthetized nude mice. Immediately after cell implantation, 100 μl of D-luciferin (30 mg/ml) was injected intraperitoneally followed by imaging with a cooled charge-coupled device (CCD) camera imaging at 1-min intervals until reaching the maximum photon counts. At the zero time point, the site implanted with the cotransfected cells exhibited significant signal (2.5 ± 0.87 × 10^5^ p/s per cm^2^ per steridian (sr)), compared to those implanted with monotransfected cells (<2.9 ± 0.7 × 10^3^ p/s per cm^2^ per sr). For comparison, the effect of the reconstitution strategy was also examined in mice in vivo. 293T cells were cotransfected with pCMV-NFluc-DnaE-n-p53 plus pCMV-MyoD-DnaE-c-CFluc. After implanted the transfected cells and injected with D-luciferin, the images were collected with a CCD camera under similar conditions. The observed signal appeared to be 10 ± 2% greater than that obtained from the complementation strategy.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( MyoD + Fluc + ID) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( MyoD + Fluc + ID) +AND+human)]

No publication is currently available.

### NIH Support

CA 86306, CA 82214, CA 92865

## References

1 Conti E., Franks N.P., Brick P. (1996). Crystal structure of firefly luciferase throws light on a superfamily of adenylate-forming enzymes. Structure.
2 Paulmurugan R., Gambhir S.S. (2005). Firefly luciferase enzyme fragment complementation for imaging in cells and living animals. Anal Chem.
3 Ray P., Pimenta H., Paulmurugan R., Berger F., Phelps M.E., Iyer M., Gambhir S.S. (2002). Noninvasive quantitative imaging of protein-protein interactions in living subjects. Proc Natl Acad Sci U S A.
4 Ozawa T. (2006). Designing split reporter proteins for analytical tools. Anal Chim Acta.
5 Weintraub H., Davis R., Tapscott S., Thayer M., Krause M., Benezra R., Blackwell T.K., Turner D., Rupp R., Hollenberg S., et al. (1991). The myoD gene family: nodal point during specification of the muscle cell lineage. Science.
6 Fong S., Debs R.J., Desprez P.Y. (2004). Id genes and proteins as promising targets in cancer therapy. Trends Mol Med.
7 Paulmurugan R., Umezawa Y., Gambhir S.S. (2002). Noninvasive imaging of protein-protein interactions in living subjects by using reporter protein complementation and reconstitution strategies. Proc Natl Acad Sci U S A.